# [N-methyl-^11^C]4-(4-(4-Chlorophenyl)-4-hydroxypiperidin-1-yl)-2,2-diphenyl-N-dimethyl-butanamide

Chemical name: | [N-methyl-^11^C]4-(4-(4-Chlorophenyl)-4-hydroxypiperidin-1-yl)-2,2-diphenyl-N-dimethyl-butanamide
Abbreviated name: | [^11^C]Lop
Synonym: | [^11^C]Loperamide
Agent category: | Compound
Target: | P-glycoprotein multidrug transporter, MDR-1
Target category: | Transporter
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide)]

One of the mechanisms of tumor cells to escape the cytotoxic effects of chemotherapeutic agents, such as adriamycin, vinca alkaloids, epipodophyllotoxins, actinomycin D, and paclitaxel, is to limit their presence inside the cells by way of a multidrug resistance (MDR-1) gene protein (1, 2). The MDR-1 gene encodes a transmembrane P-glycoprotein (P-gp) as an ATP-dependent multidrug transporter that is capable of actively pumping a variety of agents out of the cells. Injection of unlabeled efflux pump substrates increases the retention of the radioactivity in the tumor by blocking the efflux rather than reducing radioactivity as seen with receptor-binding radiotracer blocking studies. Overexpression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood–brain barrier (BBB) (4, 5). Calcium channel blockers, cyclosporin, and its non-immunosuppressive analog PSC 833 are MDR modulators that inhibit the transport of P-gp substrates out of the cells (6, 7).

^99m^Tc-sestamibi (MIBI) has been approved by the United States Food and Drug Administration as a myocardial perfusion imaging agent for use with single-photon emission computed tomography to assess the risk of future cardiac events (9). It is also used as a tumor-imaging agent in breast, lung, thyroid, and brain cancers (9-11). But sestamibi (MIBI) is a substrate for P-gp (4, 8). Loperamide (Lop) is an opiate agonist (12) and an avid substrate for P-gp at the BBB (13). Therefore, ^11^C-labeled Lop ([^11^C]Lop) is being developed as a positron emission tomography (PET) agent for the non-invasive study of the P-gp function and MDR in tumors and normal tissues (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20synthesis)]

[^11^C]Lop was synthesized by reaction of 4-(4-(4-chlorophenyl)-4-hydroxypiperidin-1-yl)-2,2-diphenyl-N-methyl-butanamide (dLop) with [^11^C]methyl iodide for 6 min at 80°C (14). The radiochemical purity of purified [^11^C]Lop was >99% with specific activities of 42.6 ± 23.9 GBq/µmol (1.15 ± 0.65 Ci/µmol) at the end of synthesis. The total synthesis time was 37 min with a radiochemical yield of 11% (decay-corrected).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20in%20vitro)]

In vitro binding studies using cloned receptors with Lop exhibited inhibition constant (K_i_) values of 0.31, 47, and 116 nM for µ, δ, and κ opiate receptors, respectively (14). The measured log D_7.4_ of [^11^C]Lop was 3.04.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20rodentia)]

Biodistribution studies with [^11^C]Lop with PET imaging in normal and P-gp knockout mice showed 2.7-fold and 1.9-fold higher accumulation of radioactivity in the forebrain and cerebellum, respectively, in the knockout mice than in the wild-type mice (14). Four radiometabolites were detected with high-performance liquid chromatography (HPLC) in the plasma and brains. The most lipophilic radiometabolite was putatively found to be dLop on HPLC. In the knockout mice, the fraction of unchanged [^11^C]Lop in the plasma and brain as determined with HPLC was 22% and 50%, respectively, at 60 min after injection. In the wild-type mice, the fraction of unchanged [^11^C]Lop in the plasma and brain was 25% and 13%, respectively, at 60 min after injection. The ex vivo brain concentrations of [^11^C]Lop and [^11^C]dLop were ~16-fold greater in the knockout mice than in the wild-type mice, whereas no differences were observed in the plasma of these mice. There was a 4-fold increase in total radioactivity ([^11^C]Lop plus its radiometabolites) in the forebrain in the knockout mice as compared with the wild-type mice. No studies with known P-gp blockers were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20%28nonhuman%20primate%29)]

Zoghbi et al. (14) showed that pretreatment with DCPQ and tariquidar (P-gp blockers) in three rhesus monkeys enhanced brain [^11^C]Lop PET radioactivity by 3.7-fold and 3-fold, respectively. The increase in brain radioactivity was not caused peripherally because DCPQ and tariquidar insignificantly changed the plasma concentration and plasma protein binding of [^11^C]Lop as well as metabolism prolife of [^11^C]Lop. At least six radiometabolites were detected in monkey arterial plasma at 15 min after injection. One of the metabolites was putatively found with HPLC to be dLop (2.6%). Demethylation of [^11^C]Lop to [^11^C]dLop precludes quantification of the P-gp function with PET if [^11^C]dLop is also an avid substrate for P-gp. Also, the number of metabolites in the brain, when only 511 keV gamma rays are being detected also confounds the interpretation.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20%28%20human%29)]

No publications are currently available.

## NIH Support

Intramural research program

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Thiebaut F., Tsuruo T., Hamada H., Gottesman M.M., Pastan I., Willingham M.C. (1987). Cellular localization of the multidrug-resistance gene product P-glycoprotein in normal human tissues. Proc Natl Acad Sci U S A.
6 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
7 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
8 Piwnica-Worms D., Kronauge J.F., Holman B.L., Lister-James J., Davison A., Jones A.G. (1988). Hexakis(carbomethoxyisopropylisonitrile) technetium(I), a new myocardial perfusion imaging agent: binding characteristics in cultured chick heart cells. J Nucl Med.
9 Olszowska M., Kostkiewicz M., Tracz W., Przewlocki T. (2003). Assessment of myocardial perfusion in patients with coronary artery disease. Comparison of myocardial contrast echocardiography and 99mTc MIBI single photon emission computed tomography. Int J Cardiol.
10 Benard F., Romsa J., Hustinx R. (2003). Imaging gliomas with positron emission tomography and single-photon emission computed tomography. Semin Nucl Med.
11 Peng N.J., Chang H.T., Tsay D.G., Liu R.S. (2003). Technetium-99m-sestamibi scintimammography to detect breast cancer in patients with paraffinomas or siliconomas after breast augmentation. Cancer Biother Radiopharm.
12 Awouters F., Megens A., Verlinden M., Schuurkes J., Niemegeers C., Janssen P.A. (1993). Loperamide. Survey of studies on mechanism of its antidiarrheal activity. Dig Dis Sci.
13 Sadeque A.J., Wandel C., He H., Shah S., Wood A.J. (2000). Increased drug delivery to the brain by P-glycoprotein inhibition. Clin Pharmacol Ther.
14 Zoghbi S.S., Liow J.S., Yasuno F., Hong J., Tuan E., Lazarova N., Gladding R.L., Pike V.W., Innis R.B. (2008). 11C-loperamide and its N-desmethyl radiometabolite are avid substrates for brain permeability-glycoprotein efflux. J Nucl Med.